# ^89^Zr-Desferrioxamine B-J591 anti-prostate-specific membrane antigen monoclonal antibody

Chemical name: | ^89^Zr-Desferrioxamine B-J591 anti-prostate-specific membrane antigen monoclonal antibody
Abbreviated name: | ^89^Zr-DFO-J591
Synonym:
Agent category: | Antibody
Target: | Prostate-specific membrane antigen (PSMA), or N-acetyl α-linked acidic dipeptidase (NAALADase)
Target category: | Antigen
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^89^Zr
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4758398), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=4758397) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2346) for more information about PSMA.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Zr%20J591)]

Prostate-specific membrane antigen (PSMA) is a cell-surface glycoprotein with a molecular weight of ~100 kDa. It is a unique, type II, transmembrane-bound glycoprotein that is overexpressed on prostate tumor cells and in the neovasculature of most solid prostate tumors, but not in the vasculature of normal tissues (1, 2). PSMA has also been detected in other tissues such as the kidneys, the proximal small intestine, and the salivary glands (2). PSMA was found to have N-acetyl α-linked acidic dipeptidase (NAALADase) or glutamate carboxypeptidase II activity (3). PSMA may play an important role in the progression of prostate cancer and glutamatergic neurotransmission, as well as in the absorption of folate (4). In the central nervous system, PSMA metabolizes N-acetyl-aspartyl-glutamate, and in the proximal small intestine it removes γ-linked glutamates from poly-γ-glutamate folate and folate hydrolase (2). PSMA can be used as a marker for the detection of metastatic cancers with imaging agents. Although a commercially available monoclonal antibody (^111^In-labeled Capromomab pendetide (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=Capromab111In) (^111^In-CYT-356)) is in clinical use for the detection of prostate cancer, the results obtained with this antibody are not entirely reliable (5). In addition, this antibody has limited access to tumors and may produce low signal/noise ratios because the target is the intracellular domain of PSMA (6, 7). J591, a monoclonal antibody against the extracellular domain of PSMA, has been humanized, and the humanized J591 was conjugated with desferrioxamine B (DFO) and radiolabeled with ^89^Zr to form ^89^Zr-DFO-J591 for imaging PSMA expression in prostate tumors (8). ^89^Zr-DFO-J591 exhibited high specific binding and tumor/muscle contrast in positron emission tomography (PET) imaging in PSMA-positive prostate tumors in nude mice.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=PSMA+AND+micad%5Bbook%5D)
- Gene information in NCBI (PSMA (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=2346))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/602640)
- Clinical trials (PSMA (http://www.clinicaltrials.gov/ct2/results?term=PSMA))
- Drug information in FDA (Capromomab pendetide (http://google2.fda.gov/search?q=Capromab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=9&y=7))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Zr%20J591%20AND%20synthesis)]

J591 was coupled with N-SucDf via an amide linkage (8). DFO-J591 was labeled with ^89^Zr-oxalate for ~60 min at room temperature with a high yield of >77%. ^89^Zr-DFO-J591 was purified with gel filtration. The radiochemical purity was >99% with >95% immunoreactivity. Maximum specific activity was ~27 MBq/nmol (0.73 mCi/nmol). There were ~4 DFO chelates per J591 molecule. ^89^Zr-DFO-J591 showed <2% loss of ^89^Zr and ~17% loss of immunoreactivity in 1% bovine serum albumin for 7 d at 37°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Zr%20J591%20AND%20in%20vitro)]

LNCaP human prostate cancer cells were reported to have a K_d_ value of 1.83 nM with ^131^I-labeled J591 and a B_max_ of 600,000–800,000 sites/cell in a saturation binding assay (9).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Zr%20J591%20and%20rodentia)]

Holland et al. (8) performed ex vivo biodistribution studies with 0.55–0.74 MBq (0.015–0.02 mCi) ^89^Zr-DFO-J591 (~0.026 nmol/mouse) in nude mice (n = 3–5 per group) bearing xenografts of the LnCaP (PSMA-positive) and PC-3 (PSMA-low) tumor cell lines. The uptake in the LnCaP tumors was 34.4 ± 3.2% injected dose per gram (ID/g), 38.0 ± 6.2% ID/g, 40.4 ± 4.8% ID/g, and 45.8 ± 3.2% ID/g at 24, 48, 96, and 144 h after injection, respectively. The tissue with the highest accumulation was the spleen (24.6% ID/g), followed by the liver (17.2% ID/g), bone (8.7% ID/g), kidney (5.1% ID/g), lung (2.2% ID/g), heart (1.7% ID/g), blood (1.4% ID/g), and muscle (0.4% ID/g) at 96 h after injection. The tumor/blood and tumor/muscle ratios were 30 and 96, at 96 h, respectively. Coinjection with excess J591 reduced the tumor uptake by >70% at 48 h after injection. The uptake in the PC-3 tumors was 15.6 ± 2.1% ID/g and 24.0 ± 2.6% ID/g at 48 and 96 h, respectively. The tumor/blood and tumor/muscle ratios were 2 and 25, at 96 h, respectively. Coinjection with excess J591 reduced the tumor uptake by 34% at 48 h after injection. PET imaging in nude mice (n = 3) with ~11 MBq (0.3 mCi) ^89^Zr-DFO-J591 (~0.4 nmol per mouse) visualized the LnCaP tumor as early as 24 h after injection with a maximum contrast at 144 h. The tumor/muscle ratio increased from 13.7 at 24 h to 25.9 at 144 h. On the other hand, the PC-3 tumor/muscle ratio increased only slightly from 3.7 at 24 h to 4.9 at 144 h.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Zr%20J591%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Zr%20J591%20AND%20Primates)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Zr%20J591%20AND%20human)]

No publication is currently available.

## NIH Support

U24 CA83084, P30 CA08748

## References

1 Feneley M.R., Jan H., Granowska M., Mather S.J., Ellison D., Glass J., Coptcoat M., Kirby R.S., Ogden C., Oliver R.T., Badenoch D.F., Chinegwundoh F.I., Nargund V.H., Paris A.M., Britton K.E. (2000). Imaging with prostate-specific membrane antigen (PSMA) in prostate cancer. Prostate Cancer Prostatic Dis.
2 Ghosh A., Heston W.D. (2004). Tumor target prostate specific membrane antigen (PSMA) and its regulation in prostate cancer. J Cell Biochem.
3 Luthi-Carter R., Barczak A.K., Speno H., Coyle J.T. (1998). Molecular characterization of human brain N-acetylated alpha-linked acidic dipeptidase (NAALADase). J Pharmacol Exp Ther.
4 O'Keefe, D., D. Bachich, and W.D. Heston, Prostate specific membrane antigen. Prostate cancer, biology, genetics, and the new therapeutics., ed. L. Chung, W. Issacs, and J. Simons. 2001, New Jersey: Humana Press. 307-326.
5 Ponsky L.E., Cherullo E.E., Starkey R., Nelson D., Neumann D., Zippe C.D. (2002). Evaluation of preoperative ProstaScint scans in the prediction of nodal disease. Prostate Cancer Prostatic Dis.
6 Sundaresan G., Yazaki P.J., Shively J.E., Finn R.D., Larson S.M., Raubitschek A.A., Williams L.E., Chatziioannou A.F., Gambhir S.S., Wu A.M. (2003). 124I-labeled engineered anti-CEA minibodies and diabodies allow high-contrast, antigen-specific small-animal PET imaging of xenografts in athymic mice. J Nucl Med.
7 Jain R.K. (1999). Transport of molecules, particles, and cells in solid tumors. Annu Rev Biomed Eng.
8 Holland J.P., Divilov V., Bander N.H., Smith-Jones P.M., Larson S.M., Lewis J.S. (2010). 89Zr-DFO-J591 for immunoPET of prostate-specific membrane antigen expression in vivo. J Nucl Med.
9 Smith-Jones P.M., Vallabahajosula S., Goldsmith S.J., Navarro V., Hunter C.J., Bastidas D., Bander N.H. (2000). In vitro characterization of radiolabeled monoclonal antibodies specific for the extracellular domain of prostate-specific membrane antigen. Cancer Res.